# 1-(2'-Deoxy-2'-[^18^F]fluoro-β-D-arabinofuranosyl)-5-iodocytosine

Chemical name: | 1-(2'-Deoxy-2'-[^18^F]fluoro-β-D-arabinofuranosyl)-5-iodocytosine | [image]
Abbreviated name: | ^18^F-FIAC | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Herpes simplex virus type 1 thymidine kinase (HSV1-tk) | [image]
Target Category: | Enzyme (reporter gene) | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^18^F-FIAC, ^18^F-FIAU, and ^18^F-FEAU (1, 2).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=HSV1-tk%20gene%20and%20expression%20and%20imaging)]

The ^18^F-labeled 1-(2'-deoxy-2'-[^18^F]fluoro-β-D-arabinofuranosyl)-5-iodocytosine, abbreviated as ^18^F-FIAC, is a cytidine analog synthesized for positron emission tomography (PET) of herpes simplex virus (HSV) type 1 thymidine kinase (HSV1-tk) gene expression (1, 3).

The HSV1-tk reporter gene expression was first explored with radiolabeled nucleoside analogs by Tjuvajev et al. in 1995 to monitor the activity of HSV1-tk (4). This study opened a new field of imaging of HSV1-tk gene expression in gene therapy of cancer (2, 5). Since then, a large number of radiolabeled nucleoside analogs have been reported for PET imaging of HSV1-tk reporter gene expression (2, 3). These analogs have been developed on the basis of their antiviral properties against HSV for treatment of HSV encephalitis, which involves monophosphorylation of the nucleoside analogs by HSV1-tk to their monophosphates that are subsequently converted to their di- and tri-phosphates by host kinases (1). Basically, these analogs can be divided into two major classes: pyrimidine and purine nucleoside analogs (2). The pyrimidine analogs are 2'-^18^F-fluoroarabinofuranisyluracil derivatives and a few other 5- and 6-substituted uracil derivatives. The purine analogs are fluorinated guanosine (acycloguanosine) derivatives. Pyrimidine analogs have two advantages over the guanosine analogs. First, pyrimidine nucleosides are more sensitive (by orders of magnitude) to HSV1-tk than guanosine nucleosides. Second, pyrimidine analogs are mainly cleared via the kidneys; therefore, the background activity is negligible, whereas most guanosine nucleosides are cleared through the hepatobiliary system, which leads to high radioactivity in the intestine. However, pyrimidine analogs are substrates of thymidine phosphorylase (TPase), and the glycosilic bond between the sugar and the base in the structure can be cleaved by TPase, whereas guanosine analogs are resistant to TPase; therefore, guanosine nucleosides often exhibit better tracer kinetics in this respect than the pyrimidine nucleosides. In addition, because guanosine nucleosides are not TPase substrates, they are more attractive for PET imaging of mutated HSV1-tk reporter gene expression (6).

FIAC is a potent inhibitor of HSV virus replication. In virus-infected cells, FIAC is transformed to mono-, di-, or tri-phosphate form and incorporated into the viral DNA sequence to cause anti-viral effects at concentrations as low as 10 nM (7, 8). At the same time, FIAC exhibits limited cytotoxicity (IC_50_ = 21.7 μM) to untransfected cells, indicating that FIAC might not be a proper substrate for the host thymidine kinase (8). These findings imply that FIAC might be an ideal probe for targeting HSV1-tk gene expression in living subjects. Chan et al. (1) tested the feasibility of ^18^F-FIAC as a PET radiotracer for HSV1-tk gene imaging and compared it with two highly promising thymidine analogs, 2'-deoxy-2'-[^18^F]fluoro-5-iodo-1-β-D-arabinofuranosyluracil (^18^F-FIAU) and 2'-deoxy-2'-[^18^F]fluoro-5-ethyl-1-β-D-arabinofuranosyluracil (^18^F-FEAU) (9) in an NG4TL4-WT/STK sarcoma-bearing mouse model. This chapter summarizes the data obtained with ^18^F-FIAC.

### Related Resource Links:

Probers for gene reporter expression imaging in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=gene+reporter+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

HSV-related clinical trials (http://clinicaltrials.gov/ct2/results?term=HSV)

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=HSV) and protein (http://www.ncbi.nlm.nih.gov/protein/?term=HSV) sequences of HSV

HSV-related compounds and proteins in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=HSV)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21982570)]

Wu et al. described the synthesis of ^18^F-FIAC in detail, which started from 2-O-(trifluoromethylsulfonyl)-1,3,5,-tri-O-ben-zoyl-a-D-ribofuranose (compound 1) (3). Fluorination of compound 1 with n-Bu_4_N^18^F resulted in the production of 2-deoxy-2-[^18^F]fluoro-1,3,5-tri-O-benzyl-a-D-arabinofuranose (compound 2). The radiochemical yield of compound 2 was >47%. ^18^F-FIAC was then synthesized on the basis of compound 2. ^18^F-FIAU and ^18^F-FEAU were prepared according to the methods published previously. The radiochemical yields of the three tracers were 10%–20%, with radiochemical purities >98%. The total synthetic time for each tracer was ~3.5 h. The specific activities were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21982570)]

The in vitro accumulation studies of ^18^F-FIAC, ^18^F-FIAU, and ^18^F-FEAU were conducted with HSV1-tk-positive NG4TL4-TK [tk(+)] cells and HSV1-tk-negative NG4TL4-TK [tk(–)] cells (1). Cellular uptake was expressed as cell/medium (C/M) ratio. In general, the accumulation of all three tracers in HSV1-tk-positive cells increased linearly with time. The tk(+) cells exhibited a more rapid and higher uptake of ^18^F-FIAU and ^18^F-FEAU than of ^18^F-FIAC. The C/M ratios of ^18^F-FIAC, ^18^F-FIAU, and ^18^F-FEAU in tk(+) cells after 120 min of incubation were 95.88 ± 32.21, 304.38 ± 47.78, and 281.78 ± 20.65, respectively. The tk(−) cells showed a moderate accumulation of ^18^F-FIAU (3.99 ± 0.72) but only a limited uptake of ^18^F-FIAC (1.44 ± 0.24) and ^18^F-FEAU (1.14 ± 0.15) after incubation for 2 h. The tk(+)/tk(−) cellular uptake ratios of ^18^F-FIAC, ^18^F-FIAU, and ^18^F-FEAU after 120 min incubation were 66.6 ± 25.1, 76.3 ± 18.2, and 247.2 ± 37.2, respectively. ^18^F-FIAC exhibited similar HSV1-tk specificity compared with ^18^F-FIAU. High correlations were observed between the cellular uptake of ^18^F-FIAC, ^18^F-FIAU (R^2^ = 0.99; P <0.05), and ^18^F-FEAU (R^2^ = 0.99; P <0.005), which suggested that ^18^F-FIAC behaved as an HSV1-tk gene expression probe, similar to ^18^F-FIAU and ^18^F-FEAU (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21982570)]

The biodistribution of the three tracers was analyzed in FVB/N mice bearing both HSV1-tk-positive NG4TL4-TK [tk(+)] and HSV1-tk-negative NG4TL4-TK [tk(–)] tumors after tail vein injection of 1.85 MBq (0.05 mCi) of each tracer (1). Mice were euthanized at different time points (n = 4 mice/time point per tracer). The accumulation in each tissue was expressed as the percentage of injection dose per gram of tissue (% ID/g) (Table 1).

The biodistribution results showed that the accumulations of the three tracers in tk(+) tumors were much higher than the accumulation in tk(−) tumors and in most normal organs except for kidneys (Table 1). The tk(+) tumor uptake of ^18^F-FIAC and ^18^F-FIAU increased with time after injection. The tk(+) tumor uptake of ^18^F-FEAU was lower than that of ^18^F-FIAC and ^18^F-FIAU. However, the tk(+)/tk(−), tk(+)/muscle, and tk(+)/blood ratios for ^18^F-FEAU were much higher than those for ^18^F-FIAC and ^18^F-FIAU, which may be due to the rapid blood clearance and fast urine excretion of ^18^F-FEAU compared with ^18^F-FIAC and ^18^F-FIAU. The distribution profile of ^18^F-FIAC was similar to that of ^18^F-FIAU but was different from that of ^18^F-FEAU. The high radioactivity in the kidney and urine indicated that all three tracers and their radioactive metabolites were mainly excreted via the urinary system.

Table 1: Accumulation of the tracers in selected organs 120 min after injection.

Tracer | Blood | Liver | Kidney | Bone | tk(+) | tk(–) | tk(+)/tk(−) | tk(+)/M | tk(+)/Blood
^18^F-FIAC | 2.71 | 3.47 | 4.54 | 1.18 | 51.59 | 4.11 | 12.6 | 21.9 | 19
^18^F-FIAU | 2.53 | 2.51 | 4.18 | 0.76 | 58.55 | 3.71 | 15.8 | 26.9 | 23.1
^18^F-FEAU | 0.34 | 0.27 | 0.52 | 0.68 | 14.56 | 0.30 | 48.0 | 42.8 | 42.8

tk(+), tk(−), and tk(+)/M represent HSV1-tk-positive, HSV1-tk-negative, and tk(+)/muscle ratio, respectively.

Analysis of the radioactive metabolites in urine at 30 min after injection of ^18^F-FIAC in tumor-bearing mice showed that intact ^18^F-FIAC only accounted for 4% of radioactivity in the urine, and the radioactivity of other metabolites including 1-(2'-deoxy-2'-[^18^F]fluoroarabinofuranosyl)cytosine (^18^F-FAC), ^18^F-FIAU, and (1-(2'-deoxy-2'-fluoro-beta-D-arabinofuranosyl)uracil (^18^F-FAU) was 24%, 48%, and 2%, respectively. ^18^F-FIAC may be regarded as the prodrug of ^18^F-FIAU in vivo (1).

MicroPET scanning of the tk(+)/tk(−) tumor-bearing mice was conducted at 1 h after injection of 1.11 MBq (0.03 mCi) ^18^F-FIAC, ^18^F-FIAU, and ^18^F-FEAU on three consecutive days (1). The tk(+) tumor was clearly delineated with high contrast in the PET images. The tk(+)/muscle ratio was 5.5 for ^18^F-FIAC, 10.8 for ^18^F-FIAU, and 7.0 for ^18^F-FEAU. The tk(+)/tk(−) tumor uptake ratios were 4.8 for ^18^F-FIAC, 6.7 for ^18^F-FIAU, and 7.0 for ^18^F-FEAU. These results were consistent with the results observed in the biodistribution studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Chan P.C., et al. (2011). Evaluation of F-18-labeled 5-iodocytidine (18F-FIAC) as a new potential positron emission tomography probe for herpes simplex virus type 1 thymidine kinase imaging. Nucl Med Biol.
2 Alauddin M.M., Gelovani J.G. (2010). Radiolabeled nucleoside analogues for PET imaging of HSV1-tk gene expression. Curr Top Med Chem.
3 Wu C.Y., et al. (2009). Radiosynthesis of F-18 labeled cytidine analog 2'-fluoro-5-iodo-l-beta-d-arabinofuranosylcytosine ([(18)F]FIAC). Appl Radiat Isot.
4 Tjuvajev J.G., et al. (1995). Imaging the expression of transfected genes in vivo. Cancer Res.
5 Blasberg R.G., Tjuvajev J.G. (1999). Herpes simplex virus thymidine kinase as a marker/reporter gene for PET imaging of gene therapy. Q J Nucl Med.
6 Najjar A.M., et al. (2009). Molecular-genetic PET imaging using an HSV1-tk mutant reporter gene with enhanced specificity to acycloguanosine nucleoside analogs. J Nucl Med.
7 Lopez C., Watanabe K.A., Fox J.J. (1980). 2'-fluoro-5-iodo-aracytosine, a potent and selective anti-herpesvirus agent. Antimicrob Agents Chemother.
8 Schinazi R.F., et al. (1986). Activities of 1-(2-deoxy-2-fluoro-beta-D-arabinofuranosyl)-5-iodocytosine and its metabolites against herpes simplex virus types 1 and 2 in cell culture and in mice infected intracerebrally with herpes simplex virus type 2. Antimicrob Agents Chemother.
9 Alauddin M.M., et al. (2007). In vivo evaluation of 2'-deoxy-2'-[(18)F]fluoro-5-iodo-1-beta-D-arabinofuranosyluracil ([18F]FIAU) and 2'-deoxy-2'-[18F]fluoro-5-ethyl-1-beta-D-arabinofuranosyluracil ([18F]FEAU) as markers for suicide gene expression. Eur J Nucl Med Mol Imaging.